# Cy5.5-Asp-Gly-Glu-Ala (DGEA)

Chemical name: | Cy5.5-Asp-Gly-Glu-Ala (DGEA)
Abbreviated name: | Cy5.5-DGEA
Synonym:
Agent category: | Peptide
Target: | Integrin α_2_β_1_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA)]

Integrin receptors are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events (e.g., cell adhesion, migration, differentiation, proliferation, and apoptosis) involving cell–cell and cell–matrix interactions (1, 2). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. On the other hand, integrins affect tumor growth, tumor invasiveness, and metastasis (3, 4). The α_2_β_1_ integrin binds mainly to collagen type I, laminins, E-cadherin, and matrix metalloproteinase 1 (5). The α_2_β_1_ integrin is strongly expressed on tumor cells and has been implicated in tumor progression and metastasis (6, 7). In particular, prostate cancer cells and prostate cancer stem cells express high levels of α_2_β_1_ integrin (8, 9). A tetrapeptide sequence consisting of Asp-Gly-Glu-Ala (DGEA) has been identified as a recognition motif used by the type I collagen to bind to α_2_β_1_ integrin (10). DGEA was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in prostate tumor-bearing mice (11). Cy5.5-DGEA exhibited high accumulation in α_2_β_1_-positive PC-3 human prostate tumor cells in nude mice.

### Related Resource Links:

- Chapters in MICAD (DGEA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=DGEA+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_2_ integrin (http://www.ncbi.nlm.nih.gov/gene/3673), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_2_ integrin (http://www.ncbi.nlm.nih.gov/omim/192974), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+synthesis)]

DGEA peptides were obtained using solid-phase synthesis (11). Cy5.5-N-hydroxysuccinimide (NHS) ester was used to conjugate DGEA peptides using solid-phase synthesis to form Cy5.5-DGEA. The NHS ester of Cy5.5 reacted with the N-terminal amino group of the Asp of the DGEA peptides. The measured mass of Cy5.5-DGEA was m/z 1,287.3, which was ~1 Cy5.5/DGEA. The chemical purity was >98%. Cy5.5 is a NIR fluorescence dye with absorbance maximum at 675 nm and emission maximum at 694 nm, with a high extinction coefficient of 250,000 M−^1^cm−^1^. 5-Carboxyfluorescin-DGEA (FAM-DGEA) peptides were similarly prepared for in vitro studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+and+in+vitro)]

Flow cytometry analysis showed that 99.7% of PC-3 cells, 51.4% of CWR-22 cells, and 15.6% of LNCaP cells were positive for the α_2_β_1_ receptors using FAM-DGEA (11). Binding of 1 µM FAM-DGEA to the three cell types was analyzed with fluorescence microscopy. PC-3 cells exhibited a higher fluorescence intensity signal than CWR-22 and LNCaP cells. The binding of FAM-DGEA to PC-3 cells could be completely blocked with 20 µM DGEA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+rodentia)]

Huang et al. (11) performed NIR fluorescence imaging of nude mice (n = 3) bearing PC-3 tumors at 0.5–24 h after intravenous injection of 1.3 nmol Cy5.5-DGEA. The tumor accumulation of Cy5.5-DGEA could be clearly visualized from 1 h to 24 h, with a maximum contrast at 2 h. The tumor/background ratio was ~10 at 2 h after injection. Co-injection of 300 nmol DGEA inhibited the signal by 40% at 4 h after injection. This low reduction of signal may be due to non-specific binding in the tumor. There was also some reduction of signal in the liver, lung, spleen, and muscle due to normal expression of α_2_β_1_ integrin in these tissues. Ex vivo imaging of tissues at 28 h after injection showed that the tissues with highest signal were the tumor and kidney, followed by the liver, lung, pancreas, spleen, muscle, and heart. Immunohistochemistry staining of PC-3 tumor sections showed a strong expression of α_2_β_1_ integrin in the tumor cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=DGEA+human)]

No publication is currently available.

## References

1 Hynes R.O. (2009). The extracellular matrix: not just pretty fibrils. Science.
2 Barczyk M., Carracedo S., Gullberg D. (2010). Integrins. Cell Tissue Res.
3 Makrilia N., Kollias A., Manolopoulos L., Syrigos K. (2009). Cell adhesion molecules: role and clinical significance in cancer. Cancer Invest.
4 Brooks S.A., Lomax-Browne H.J., Carter T.M., Kinch C.E., Hall D.M. (2010). Molecular interactions in cancer cell metastasis. Acta Histochem.
5 Heino J. (2000). The collagen receptor integrins have distinct ligand recognition and signaling functions. Matrix Biol.
6 Barbolina M.V., Moss N.M., Westfall S.D., Liu Y., Burkhalter R.J., Marga F., Forgacs G., Hudson L.G., Stack M.S. (2009). Microenvironmental regulation of ovarian cancer metastasis. Cancer Treat Res.
7 Kirkland S.C., Ying H. (2008). Alpha2beta1 integrin regulates lineage commitment in multipotent human colorectal cancer cells. J Biol Chem.
8 Hall C.L., Dai J., van Golen K.L., Keller E.T., Long M.W. (2006). Type I collagen receptor (alpha 2 beta 1) signaling promotes the growth of human prostate cancer cells within the bone. Cancer Res.
9 Kiefer J.A., Farach-Carson M.C. (2001). Type I collagen-mediated proliferation of PC3 prostate carcinoma cell line: implications for enhanced growth in the bone microenvironment. Matrix Biol.
10 Staatz W.D., Fok K.F., Zutter M.M., Adams S.P., Rodriguez B.A., Santoro S.A. (1991). Identification of a tetrapeptide recognition sequence for the alpha 2 beta 1 integrin in collagen. J Biol Chem.
11 Huang C.W., Li Z., Conti P.S. (2011). In Vivo Near-Infrared Fluorescence Imaging of Integrin alpha2beta1 in Prostate Cancer with Cell-Penetrating-Peptide-Conjugated DGEA Probe. J Nucl Med.